# (2S,3S)-N-[[2-[^11^C]Methoxy-5-[5-(trifluoromethyl)tetrazol-1-yl]phenyl]methyl]-2-phenyl-piperidin-3-amine

Chemical name: | (2S,3S)-N-[[2-[^11^C]Methoxy-5-[5-(trifluoromethyl)tetrazol-1-yl]phenyl]methyl]-2-phenyl-piperidin-3-amine
Abbreviated name: | [^11^C]GR205171
Synonym:
Agent Category: | Compound
Target: | NK_1_ receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DGR205171%20OR%20%28NK1%20PET%20ligand%29)]

(2S,3S)-N-[[2-[^11^C]Methoxy-5-[5-(trifluoromethyl)tetrazol-1-yl]phenyl]methyl]-2-phenyl-piperidin-3-amine ([^11^C]GR205171) is a radioligand developed for positron emission tomography (PET) imaging of NK_1_ receptors (substance P (SP) receptors) in the central nervous system (CNS) (1).

Tachykinins are peptides comprising 10 to12 amino acids that share a common carboxy-terminal sequence “Phe-X-Gly-Leu-Met-amide” where “X” is different but always a hydrophobic residue that is either an aromatic or a beta-branched aliphatic (2-4). This peptide family consists of SP, neurokinin A (NK_A_), and neurokinin B (NK_B_). The tachykinin peptides mediate their effects by specific G protein-coupled receptors. These receptors are divided into three subtypes: neurokinin 1 (NK_1_, formerly the SP receptor), neurokinin 2 (NK_2_, formerly the substance K/substance E receptor/NK_A_ receptor), and neurokinin 3 (NK_3_, formerly the NK_B_ receptor). The effects of SP are mediated primarily via the NK_1_ receptor subtypes. There is evidence that SP behaves like a neurotransmitter involved in regulation of emotional and behavioral responses to a range of noxious and stressful stimuli (5). SP may also play a role in neurogenic inflammation, vasomotor control, and many gastrointestinal functions. Studies in the brain have shown that in the brain SP is found in the neocortex, in limbic areas, habenula, periaqueductal gray matter, midbrain nuclei, and is especially enriched in the basal ganglia. There is little SP in the cerebellum. The distribution of the NK_1_ receptors in the brain generally corresponds to that of SP.

SP-NK_1_ receptor pathways are found in both the CNS and the peripheral nervous system. The CNS pathways have been implicated in the pathophysiology of pain, nausea/emesis, and depression disorders (6). PET and single-photon emission tomography of radioligands targeting NK_1_ receptors can visualize and allow the study of CNS NK_1_ receptors in normal and pathologic states. These studies can identify the degree of receptor occupancy in patients with depression and the change in response to therapy (6). A number of NK_1_ selective agonists and antagonists have been successfully labeled, but they failed to provide a specific signal in vivo (6, 7). Solin et al. (7) developed a selective NK_1_ receptor antagonist, SPA-RQ, with a high affinity for NK_1_ receptor. Gardner et al. (8) reported the discovery of a trifluoromethyl compound, GR205171, as a potent NK_1_ receptor antagonist. This compound has a high affinity for the human NK1 receptor and has a high degree of selectivity and specificity. ^11^C-labeled GR205171 shows promising potential to be used as a PET ligand to characterize NK_1_-receptor binding (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DGR205171%20OR%20%28NK1%20PET%20ligand%29%29%20AND%20synthesis%5BAll%20Fields%5D)]

Ward et al. (9) reported the synthesis of GR203040, a tetrazolyl-substituted analogue of CP-99,994 (10). Gardner et al. (8) prepared GR205171 by trifluoromethyl substitution at the C-1 position of the GR203040 tetrazole moiety. Radiosynthesis of [^11^C]GR205141 was conducted by dissolving GR205141 in dichloromethane (1). Tetrabutylammonium hydroxide was added, and the mixture was heated and shaken for 2 min. After the solvent was evaporated, the residue was redissolved in N,N-dimethylformamide. [^11^C]methyl iodide was trapped in this solution at room temperature. The mixture was then heated at 80ºC for 5 min. [^11^C]GR205141 was obtained and purified by high performance liquid chromatography. The radiochemical yield was 45% based on [^11^C]methyl iodide with a total synthesis time of 45 min. The radiochemical purity was >98%, and the specific activity was 20-120 GBq/ μmol. (0.54-3.24 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DGR205171%20OR%20%28NK1%20PET%20ligand%29%29%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

Gardner et al. (8) studied the in vitro NK_1_ receptor binding affinity of GR205171 in the rat cortex membrane, ferret cortex membrane, and human Chinese hamster ovary (CHO) cells (expressing human recombinant NK_1_ receptors). Based on inhibition of ^3^H labeled SP binding, the pK_i_ values (n = 4−5) were calculated to be 9.5 ± 0.15, 9.8 ± 0.13, and 10.6 ± 0.22 for the rat cortex membrane, ferret cortex membrane, and human CHO cells, respectively. In comparison, the pK_i_ values of CP-99,994 and GR203040 for the human NK_1_ receptors were 9.6 ± 0.1 (n = 20) and 10.3 ± 0.1 (n = 4−5), respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DGR205171%20OR%20%28NK1%20PET%20ligand%29%29%20AND%20%28primate%20NOT%20human%29)]

Bergstrom et al. (1) conducted PET imaging of [^11^C]GR205171 in rhesus monkeys. The monkeys were given either a low i.v. dose (10 MBq (0.27 mCi); n = 3) or a high I.v. dose (50 MBq (1.35 mCi); n = 6) of [^11^C]GR205171. The striatum had the highest level of radioactivity in all studies. The standardized uptake value (SUV) of the striatum increased from 2 at 10 min after injection to 2.8 at 50 min. The SUVs of other grey matter regions remained constant at 2. The SUV of cerebellum decreased with time. With pretreatment of the monkeys with unlabeled GR205171 (0.05 mg/kg – 1 mg/kg; n = 8) 5 min before [^11^C]GR205171 administration, the striatum could not be visually identified, and the SUV decreased from the initial 2.3 to approximately1.7 at 50 min. For the linear graphs generated from the Patlak graphical method using the cerebellum as the reference tissue without GR205171 treatment, the highest slope values were found for the striatum and the lowest slope values were in the white matter. The absence of a plateau in these graphs indicated that there was a very slow dissociation of the ligand from the receptor. There was a significant decrease in the slope values of all regions after pretreatment with GR205171. The decrease in the slope values was >80% at all doses of GR205171. The plasma radioactivity level decreased rapidly and reached a plateau at SUV 0.5 after 10 min without GR205171 pretreatment. With GR20517 pretreatment, the plasma radioactivity level increased by 50%.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No publication is currently available.

## References

1 Bergstrom M., Fasth K.J., Kilpatrick G., Ward P., Cable K.M., Wipperman M.D., Sutherland D.R., Langstrom B. (2000). Brain uptake and receptor binding of two [11C]labelled selective high affinity NK1-antagonists, GR203040 and GR205171--PET studies in rhesus monkey. Neuropharmacology.
2 Hietala J., Nyman M.J., Eskola O., Laakso A., Gronroos T., Oikonen V., Bergman J., Haaparanta M., Forsback S., Marjamaki P., Lehikoinen P., Goldberg M., Burns D., Hamill T., Eng W.S., Coimbra A., Hargreaves R., Solin O. (2005). Visualization and quantification of neurokinin-1 (NK1) receptors in the human brain. Mol Imaging Biol.
3 Severini C., Improta G., Falconieri-Erspamer G., Salvadori S., Erspamer V. (2002). The tachykinin peptide family. Pharmacol Rev.
4 Datar P., Srivastava S., Coutinho E., Govil G. (2004). Substance P: structure, function, and therapeutics. Curr Top Med Chem.
5 Mantyh P.W. (2002). Neurobiology of substance P and the NK1 receptor. J Clin Psychiatry.
6 Hargreaves R. (2002). Imaging substance P receptors (NK1) in the living human brain using positron emission tomography. J Clin Psychiatry.
7 Solin O., Eskola O., Hamill T.G., Bergman J., Lehikoinen P., Gronroos T., Forsback S., Haaparanta M., Viljanen T., Ryan C., Gibson R., Kieczykowski G., Hietala J., Hargreaves R., Burns H.D. (2004). Synthesis and characterization of a potent, selective, radiolabeled substance-P antagonist for NK1 receptor quantitation: ([18F]SPA-RQ). Mol Imaging Biol.
8 Gardner C.J., Armour D.R., Beattie D.T., Gale J.D., Hawcock A.B., Kilpatrick G.J., Twissell D.J., Ward P. (1996). GR205171: a novel antagonist with high affinity for the tachykinin NK1 receptor, and potent broad-spectrum anti-emetic activity. Regul Pept.
9 Ward P., Armour D.R., Bays D.E., Evans B., Giblin G.M., Heron N., Hubbard T., Liang K., Middlemiss D., Mordaunt J., Naylor A., Pegg N., Vinader M.V., Watson S.P., Bountra C., Evans D.C. (1995). Discovery of an orally bioavailable NK1 receptor antagonist, (2S,3S)-(2-methoxy-5-tetrazol-1-ylbenzyl)(2-phenylpiperidin-3-yl)amine (GR203040), with potent antiemetic activity. J Med Chem.
10 Livni E., Babich J.W., Desai M.C., Godek D.M., Wilkinson R.A., Rubin R.H., Fischman A.J. (1995). Synthesis of a 11C-labeled NK1 receptor ligand for PET studies. Nucl Med Biol.